# ^99m^Tc-Labeled pyridyl benzofuran derivatives to target β-amyloid plaques

Chemical name: | ^99m^Tc-Labeled pyridyl benzofuran derivatives to target β-amyloid plaques | [image]
Abbreviated name: | [^99m^Tc]BAT-bp-1, [^99m^Tc]BAT-bp-2, and [^99m^Tc]BAT-bp-3 | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | β-Amyloid plaques (βA) | [image]
Target Category: | Peptides | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of [^99m^Tc]BAT-bp-1, [^99m^Tc]BAT-bp-2, and [^99m^Tc]BAT-bp-3 according to Cheng et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=imaging%20of%20alzheimer%20s%20disease&cmd=DetailsSearch)]

In developed countries, Alzheimer’s disease (AD) affects ~1% of the individuals who are ≥65 years old and roughly 30% of those who are ≥80 years of age (2). The disease is characterized by slow deposition of the amyloid beta protein (βA) and formation of neurofibrillary tangles in the memory and cognition regions of the brain, which lead to memory loss and cognitive impairment in the individual (3). The generation of βA from its precursor, the amyloid precursor protein, has been illustrated by Tam and Pasternak (2), and the biochemistry of this protein and the amyloid deposits in AD has been discussed by Masters and Selkoe (4). Because the deposition of βA in the brain starts several years before the symptoms of AD are apparent, detection of the disease at an early stage can assist in the diagnosis, improved monitoring of the disease, and the development of a therapeutic regimen that can slow the advancement of AD (1). Although several drugs approved (http://www.alz.org/research/science/alzheimers_disease_treatments.asp?gclid=COvK06mpkrECFYao4Aodyw3ofA#approved) by the United States Food and Drug Administration (FDA) are available to treat the symptoms of AD, none of these medications prevent the onset and progression of the disease. Imaging probes for use with positron emission tomography (PET) have been evaluated under preclinical conditions for the noninvasive visualization of AD (1), and ^18^F-labeled AV45 (florbetapir (http://www.amyvid.com/pages/home.aspx)) was approved by the FDA to estimate the density of βA neuritic plaque in the brains of AD patients. Cheng et al. showed that ^18^F-labeled 5-(5-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N,N-dimethylpyridin-2-amine ([^18^F]FPYBF), a derivative of benzofuran, had a high affinity for βA plaques, can label the plaques in postmortem human AD brain sections, and is suitable for the visualization of βA deposits in brain sections of mice (a murine model of AD) injected with [^18^F]FPYBF (5). Similar observations have been reported from biodistribution studies with two other ^18^F-labeled derivatives of benzofuran (6). A common limitation of these PET imaging compounds (under development or approved by the FDA) is that the tracers have a short half-life (e.g., the half-life of the most commonly used radionuclides for PET imaging, such as ^11^C, ^18^F, and ^68^Ga, are 20.4 min, 109.8 min, and 67.6 min, respectively), may not establish the presence of βA plaques in the brain with certainty, and cannot be used to monitor the therapeutic response in an AD patient.

As an alternative to detect βA plaques with PET, investigators have evaluated the use of several ^99m^Tc-labeled compounds (half-life of ^99m^Tc is 6 h) with single-photon emission computed tomography (SPECT) (1). However, most of these radiolabeled chemicals have been used to visualize the plaques in in vitro sections of mouse and human brains with AD and do not exhibit a high affinity for the βA plaques in vivo or can not cross the blood–brain barrier (BBB) in the animals (1). On the basis of results obtained with the benzofuran derivatives mentioned above (5, 6), ^99m^Tc-labeled pyridyl benzofuran (Bp) derivatives were synthesized, and the biodistribution of these tracers was investigated in normal mice (1). To label the Bp derivatives with ^99m^Tc, a compact chelating agent, bis(aminoethanethiol) (BAT), was conjugated to the compounds to generate radiolabeled probes (designated [^99m^Tc]BAT-Bp-1, [^99m^Tc]BAT-Bp-2, and [^99m^Tc]BAT-Bp-3).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Amyloid%20plaques%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

What is Alzheimer’s disease? [PubMed Health (http://www.ncbi.nlm.nih.gov/pubmedhealth/PMH0001767/)]

Alzheimer’s disease clinical trials (http://clinicaltrials.gov/ct2/results?term=Alzheimer%27s+disease)

Human amyloid beta (A4) precursor protein; Gene ID: 351 (NCBI Gene database (http://www.ncbi.nlm.nih.gov/gene/351))

Alzheimer’s disease in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/104300))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22364445%5Buid%5D&cmd=DetailsSearch)]

The synthesis of [^99m^Tc]BAT-Bp-1, [^99m^Tc]BAT-Bp-2, and [^99m^Tc]BAT-Bp-3 (BAT-Bp-2 and BAT-Bp-3 are the N-monomethylated- and N,N-dimethylated derivatives of BAT-Bp-1, respectively) has been described by Cheng et al. (1). The radiochemical purity of these tracers was reported to be >99% as determined with high-performance liquid chromatography. The radiochemical yield and specific activity of the different probes were not reported.

For in vitro studies, rhenium (Re) complexes of the Bp derivatives (Re-BAT-Bp-1, Re-BAT-Bp-2, and Re-BAT-Bp-3) were prepared as detailed elsewhere (1). The yields of purified Re-BAT-Bp-1, Re-BAT-Bp-2, and Re-BAT-Bp-3 were 46.0%, 26.7%, and 33.0%, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22364445%5Buid%5D&cmd=DetailsSearch)]

The binding affinities of Re-BAT-Bp-1, Re-BAT-Bp-2, and Re-BAT-Bp-3 for the βA aggregates were determined in a competition assay with [^125^I]IMPY as the binding ligand (1). All the Re compounds inhibited the binding of [^125^I]IMPY to the βA aggregates in a dose-dependent manner. The inhibition constants (K_i_) of Re-BAT-Bp-1, Re-BAT-Bp-2, and Re-BAT-Bp-3 were reported to be 149.6 ± 34.4 nM, 32.8 ± 5.80 nM, and 13.6 ± 1.60 nM, respectively.

Using a 1-octanol/phosphate-buffered saline (pH 7.4) mixture, the partition coefficients (log P values) of [^99m^Tc]BAT-Bp-1, [^99m^Tc]BAT-Bp-2, and [^99m^Tc]BAT-Bp-3 were determined to be 0.68, 1.35, and 2.09, respectively, indicating that the radiolabeled compounds were probably suitable for penetration of the BBB (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22364445%5Buid%5D&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]BAT-Bp-1, [^99m^Tc]BAT-Bp-2, and [^99m^Tc]BAT-Bp-3 was investigated in normal ddY mice (http://animal.nibio.go.jp/e_ddys.html) (1). The animals (n = 5 mice/time point; under isoflurane anesthesia) were injected with 148 kBq (4 μCi) of the tracer through the tail vein and euthanized at predetermined time points ranging from 2 min postinjection (p.i.) to 60 min p.i. Organs of interest were harvested from the animals, and the amount of label accumulated in the various tissues was determined. The uptake of radioactivity in the organs was presented as percent of injected dose per gram tissue (% ID/g). [^99m^Tc]BAT-Bp-1 and [^99m^Tc]BAT-Bp-2 showed maximum uptake of tracer in the brain at 2 min p.i. (1.59 ± 0.21% ID/g and 1.80 ± 0.16% ID/g, respectively). With [^99m^Tc]BAT-Bp-3, the peak uptake of radioactivity in the brain was 1.64 ± 0.27% ID/g at 10 min p.i. Among the ^99m^Tc-labeled Bp derivatives, [^99m^Tc]BAT-Bp-2 showed the maximum uptake in the brain, and it was concluded that this labeled compound was superior to any ^99m^Tc-labeled tracer previously used for βA imaging (1).

In another study, Tg2576 transgenic mice (http://www.criver.com/en-US/ProdServ/ByType/Discovery/CNS/Alzheimers/Pages/Tg2576_Mouse.aspx) (used as a murine model of AD; number of animals not reported) and wild-type mice (number of animals not reported) under anesthesia were injected with 16.6 MBq (448.6 μCi) [^99m^Tc]BAT-Bp-2 through the tail vein (1). The rodents were euthanized at 30 min p.i., and the brains were removed, frozen immediately, and used to prepare sections for ex vivo autoradiography. After autographic examination, the brain sections were stained with thioflavin-S to confirm the presence of βA plaques in the organs. From the autoradiograms it was clear that the radioactive spots were present only in brain sections of the Tg2576 mice. Thioflavin-S staining of the autoradiographed sections confirmed that the location of the radiolabeled spots in the brain sections corresponded to the βA deposits in the tissue.

From these studies, the investigators concluded that [^99m^Tc]BAT-Bp-2 was probably suitable to detect βA plaques with SPECT in the brains of rodents with AD (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22364445%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22364445%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22364445%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Cheng Y., Ono M., Kimura H., Ueda M., Saji H. (2012). Technetium-99m labeled pyridyl benzofuran derivatives as single photon emission computed tomography imaging probes for beta-amyloid plaques in Alzheimer's brains. J Med Chem.
2 Tam J.H., Pasternak S.H. (2012). Amyloid and Alzheimer's disease: inside and out. Can J Neurol Sci.
3 Nelson P.T., Alafuzoff I., Bigio E.H., Bouras C., Braak H., Cairns N.J., Castellani R.J., Crain B.J., Davies P., Del Tredici K., Duyckaerts C., Frosch M.P., Haroutunian V., Hof P.R., Hulette C.M., Hyman B.T., Iwatsubo T., Jellinger K.A., Jicha G.A., Kovari E., Kukull W.A., Leverenz J.B., Love S., Mackenzie I.R., Mann D.M., Masliah E., McKee A.C., Montine T.J., Morris J.C., Schneider J.A., Sonnen J.A., Thal D.R., Trojanowski J.Q., Troncoso J.C., Wisniewski T., Woltjer R.L., Beach T.G. (2012). Correlation of Alzheimer disease neuropathologic changes with cognitive status: a review of the literature. J Neuropathol Exp Neurol.
4 Masters C.L., Selkoe D.J. (2012). Biochemistry of Amyloid beta-Protein and Amyloid Deposits in Alzheimer Disease. Cold Spring Harb Perspect Med.
5 Cheng Y., Ono M., Kimura H., Kagawa S., Nishii R., Saji H. (2010). A novel 18F-labeled pyridyl benzofuran derivative for imaging of beta-amyloid plaques in Alzheimer's brains. Bioorg Med Chem Lett.
6 Ono M., Cheng Y., Kimura H., Cui M., Kagawa S., Nishii R., Saji H. (2011). Novel 18F-labeled benzofuran derivatives with improved properties for positron emission tomography (PET) imaging of beta-amyloid plaques in Alzheimer's brains. J Med Chem.